# Folic acid-indocyanine green-poly(D,L-lactide-coglycolide)-lipid nanoparticles

Chemical name: | Folic acid-indocyanine green-poly(D,L-lactide-coglycolide)-lipid nanoparticles
Abbreviated name: | FA-ICG-PLGA-lipid NPs
Synonym:
Agent Category: | Nanoparticles
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Near-infrared fluorescence imaging (NIRF); optical imaging
Source of signal / contrast: | Indocyanine green
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Indocyanine%20green%20nanoparticles&cmd=DetailsSearch)]

Indocyanine green (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=c1031b17-b6e3-4153-869f-30d9c7e66bc3) (ICG) is a water-soluble tricarbocyanine dye with a near-infrared fluorescence (NIRF) absorption maximum between 600 nm and 900 nm and an emission maximum between 750 nm and 950 nm. This is the only dye that has been approved by the United States Food and Drug Administration for noninvasive NIRF imaging to determine the cardiac output, liver function, and blood flow, and to perform ophthalmic angiography in humans (1). Although ICG has wide medical application, it has several drawbacks (due to its physicochemical characteristics) that limit its use in the clinic (2, 3). Briefly, ICG is prone to aggregate and degrade in an aqueous solution and has a short half-life even when stored in the dark (t_1/2_ = 16.8 ± 1.5 h at 22°C) (2). In addition, ICG binds to plasma proteins when administered intravenously and has a blood circulation half-life of only 2–4 min (3). Moreover, the chemical structure of the dye does not allow its conjugation to antibodies or other ligands that can be used to target the probe toward specific cellular components for the detection or diagnosis of various diseases (1). In an effort to improve the stability and circulation half-life of ICG, it was enclosed in nanoparticles (NPs), but the fluorescence signal intensities generated by the various NP formulations were either equivalent to or lower than the signal intensity of the free dye (2).

Biodegradable polymer-based NPs (4) and liposomes (5) are considered to be suitable to carry drugs because these nanomaterials are easy to synthesize, are nontoxic, and can be modified on the surface for the targeted in vivo delivery of therapeutic agents and imaging probes (5). It has been shown that lipid-polymer hybrid NPs (a biodegradable polymeric core surrounded with a lipid monolayer) exhibit the combined distinctive properties of polymeric NPs and liposomes, and that the hybrid NPs can be used for the targeted delivery of drugs to cells expressing a specific membrane antigen, such as the prostate-specific membrane antigen (6). From this study, it was concluded that such nanocarriers may be used to carry hydrophobic compounds for sustained release and to increase the circulation half-life of a drug; it was also suggested that, after conjugating the hybrid NPs with an appropriate ligand on the surface, the conjugates can be targeted to deliver therapeutic drugs to specific tissues or organs in the body. On the basis of the observations described above, folic acid (FA)–conjugated poly(D,L-lactide-coglycolide) (PLGA)-lipid NPs containing ICG at the core (FA-ICG-PLGA-lipid NPs) were fabricated and evaluated for their in vitro targeting characteristics using MCF-7 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-22&Template=cellBiology) (a human mammary gland adenocarcinoma cell line), which overexpress the folate (FA) receptor (3). The fluorescence imaging properties and biodistribution of the FA-ICG-PLGA-lipid NPs were studied in nude mice bearing MCF-7 cell tumors (3).

### Related Resource Links

Folate (http://www.ncbi.nlm.nih.gov/books?term=folate%20receptor%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)and indocyanine green (http://www.ncbi.nlm.nih.gov/books?term=Indocyanine%20green%20AND%20micad%5Bbook%5D&cmd=DetailsSearch) in MICAD

Human folate receptor protein and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/X69516.1) sequences

Clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor) related to folate receptor

Clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) related to indocyanine green

Folate receptors 1 (http://omim.org/entry/136430), 2 (http://omim.org/entry/136425), and 3 (http://omim.org/entry/602469) in Online Mendelian Inheritance in Man database (OMIM)

Human folate receptor 2 in Gene (http://www.ncbi.nlm.nih.gov/gene/2350) database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FA-ICG-PLGA-lipid%20NP%20synthesis&cmd=DetailsSearch)]

The synthesis of FA-ICG-PLGA-lipid NPs has been described by Zheng et al. (3). Briefly, a single-step nanoprecipitation method was used for the self-assembly of the FA-targeted NPs. A mixture of 90%–95% phosphatidylcholine and 1,2-distearoyl-sn-glycerol-3-phosphoethanolamine-N-[folate (polyethylene glycol)-2000] (8.5/1.5 molar ratio) in an aqueous solution of ethanol was preheated to 65°C, and a PLGA/ICG solution (molar ratios not reported) was added to the lipid mixture. The mixture was incubated for 4 h at room temperature, and the unbound materials were removed by ultrafiltration to obtain the FA-ICG-PLGA-lipid NPs.

For use as controls, nontargeted NPs were also prepared with 1,2-distearoyl-sn-glycero-3-phosphoethanolamine-N-[carboxy(polyethylene glycol) 2000] (ICG-PLGA-lipid NPs) as described above (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FA-ICG-PLGA-lipid%20NP%20in%20vitro%20studies&cmd=DetailsSearch)]

The average hydrodynamic diameter of the FA-ICG-PLGA-lipid NPs was reported to be 102.4 ± 4 nm as determined with a dynamic light scattering technique, and the zeta potential of the NPs was in the range of −28 mV to −40 mV (3).

Continuous exposure of FA-ICG-PLGA-lipid NPs and ICG to illumination from a xenon lamp for 1 h was shown to decrease the fluorescence intensities of the NPs and the free dye by 48.1% and 77.7%, respectively (3). After storage for one month at 4°C, the fluorescence intensities of FA-ICG-PLGA-lipid NPs and ICG were 84.1% and 0.35% of the initial values, respectively (3). From these studies, the investigators concluded that FA-ICG-PLGA-lipid NPs had superior stability compared with the free ICG dye (3).

The FA receptor binding specificity of the FA-ICG-PLGA-lipid NPs and the ICG-PLGA-lipid NPs was investigated by exposing MCF-7 cells and A549 cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-185&Template=cellBiology) (human lung carcinoma cell line with low expression of the FA receptor) to the two types of NPs for 30 min (3). Examination of the cells under a confocal laser scanning microscope revealed that MCF-7 cells exposed to the FA-ICG-PLGA-lipid NPs emitted a higher fluorescence signal compared with the A549 cells that were treated with the same probe. In addition, both cell types showed almost no binding of the ICG-PLGA-lipid NPs. No blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FA-ICG-PLGA-lipid%20NP%20rodentia&cmd=DetailsSearch)]

The biodistribution of free ICG, ICG-PLGA-lipid NPs, and FA-ICG-PLGA-lipid NPs was investigated in nude mice bearing MCF-7 cell tumors (3). The animals (n = 3 mice/time point per probe) were administered either 64.5 nmol ICG/kg body weight or both NPs containing an equivalent amount of ICG through the tail vein, and whole-body NIRF images of the animals were acquired at 0.5, 8, and 24 h postinjection (p.i.). For ex vivo imaging, the mice were euthanized after the 24 h of imaging, and the various organs, including the tumors, were harvested from the animals. Whole-body images acquired at 0.5 h p.i. showed that the fluorescence signal was located in the liver with all the probes. At 8 h p.i., the fluorescence signal from ICG and the ICG-PLGA-lipid NPs was located primarily in the intestines; with the FA-ICG-PLGA-lipid NPs, however, the signal was present mainly in the tumor, and low-intensity fluorescence was visible in the intestines. At 24 h p.i., the signal was detected only in tumors of mice injected with the FA-ICG-PLGA-lipid NPs. Ex vivo NIRF imaging of the various organs and tumors obtained from the different groups of mice showed that with ICG the fluorescence was present only in the liver; with ICG-PLGA-lipid NPs, the signal was detected mainly in the liver followed by the kidneys, and with the FA-ICG-PLGA-lipid NPs the fluorescence was located both in the liver and the tumors. No blocking studies were reported.

From these studies, the investigators concluded that FA-ICG-PLGA-lipid NPs can probably be used as a fluoroprobe for the detection of tumors that overexpress the FA receptor in rodents (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FA-ICG-PLGA-lipid%20NP%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FA-ICG-PLGA-lipid%20NP%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FA-ICG-PLGA-lipid%20NP%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Sharma, P., N.E. Bengtsson, G.A. Walter, H.B. Sohn, G. Zhou, N. Iwakuma, H. Zeng, S.R. Grobmyer, E.W. Scott, and B.M. Moudgil, Gadolinium-Doped Silica Nanoparticles Encapsulating Indocyanine Green for Near Infrared and Magnetic Resonance Imaging. Small, 2012
2 Kirchherr A.K., Briel A., Mader K. (2009). Stabilization of indocyanine green by encapsulation within micellar systems. Mol Pharm.
3 Zheng C., Zheng M., Gong P., Jia D., Zhang P., Shi B., Sheng Z., Ma Y., Cai L. (2012). Indocyanine green-loaded biodegradable tumor targeting nanoprobes for in vitro and in vivo imaging. Biomaterials.
4 Cabane E., Zhang X., Langowska K., Palivan C.G., Meier W. (2012). Stimuli-responsive polymers and their applications in nanomedicine. Biointerphases.
5 Heneweer C., Gendy S.E., Penate-Medina O. (2012). Liposomes and inorganic nanoparticles for drug delivery and cancer imaging. Ther Deliv.
6 Zhang L., Chan J.M., Gu F.X., Rhee J.W., Wang A.Z., Radovic-Moreno A.F., Alexis F., Langer R., Farokhzad O.C. (2008). Self-assembled lipid--polymer hybrid nanoparticles: a robust drug delivery platform. ACS Nano.